# 2-[(2-chloro-2’-^18^F-fluorodiethyl)amino]-2H-1,3,2-oxazaphosphorinane-2-oxide

Chemical name: | 2-[(2-chloro-2’-^18^F-fluorodiethyl)amino]-2H-1,3,2-oxazaphosphorinane-2-oxide
Abbreviated name: | ^18^F-F-CP
Synonym: | ^18^F-Fluorocyclophosphamide; Cytoxan®, Neosar®
Agent Category: | Compound
Target: | DNA
Target Category: | Alkylation
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | Yes (by cytochrome p450 enzymes)
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cyclophosphamide&WebEnv=0wglUOoB6l08VWm28RDARm_fx6a0nl8Tbp1XtbIixO3xJcKXPlOshaLAOFzxluUxL3mvop7oTocCkr%407748428072881B60_0000SID&WebEnvRq=1)]

2-[(2-Chloro-2’-^18^F-fluorodiethyl)amino]-2H-1,3,2-oxazaphosphorinane-2-oxide (also known as fluorocyclophosphamide and abbreviated as CP) is widely used for the treatment of cancers, as an immunosuppressant in systemic rheumatic diseases, and also as an agent to mobilize stem cells during autologous stem cell transplantation and multiple sclerosis (1-4). Actually, CP is a pro-drug that must be activated by hepatic cytochrome P450 enzymes before it can generate the DNA-alkylating phosphoramide mustard and other cellular toxic species that are known to mediate its effects (5). The biotransformation pathway of CP has been described elsewhere (6, 7). Individual differences in the metabolism, including biodistribution and pharmacokinetics, of CP and its analogs are known to influence the final outcome of clinical therapy (8). Therefore, it would be helpful to know before initiating therapy with CP or its analogs whether a patient will benefit from the treatment. Also, cell lines are known to rapidly develop resistance to CP activity, and prior exposure of the cells to other alkylating agents elevates the chances of developing the CP-resistant phenotype (9, 10). Two aldehyde dehydrogenases (ALDH1A1 (http://www.genenames.org/data/hgnc_data.php?match=ALDH1A1) and ALDH3A1 (http://www.genenames.org/data/hgnc_data.php?match=ALDH3A1)) and glutathione S-transferase are known to detoxify CP and its metabolites and are involved in the development of resistance to this drug (9, 11).

Lacan et al. envisioned that knowledge regarding the biodistribution and metabolism of CP in a patient would help healthcare providers devise a suitable chemotherapeutic regimen and perhaps predict clinical outcome of the therapy for an individual (12). The investigators synthesized a radioactive fluorine (^18^F)-labeled analog of CP, ^18^F-fluorocyclophosphamide (^18^F-F-CP), to study the in vivo metabolism of CP in tumors. Instead of using the multi-step procedure available for the synthesis of the analog to generate the compound, they applied a direct halogenation exchange protocol with a commercially available precursor (12, 13). The biodistribution of ^18^F-F-CP was studied in mice bearing xenograft tumors (14).

CP (http://www.webmd.com/drugs/drug-19924-Cyclophosphamide+IV.aspx?drugid=19924&drugname=Cyclophosphamide+IV) is approved by the United States Food and Drug Administration for the treatment of a variety of cancers and is currently being evaluated in several clinical trials (http://clinicaltrials.gov/ct2/results?term=cyclophosphamide).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+Fluorocyclophosphamide+synthesis&WebEnv=0PV8obXgHyvu-QQ0xnOmo6J3Jqhp3fMbQab0zpnQzRaJlghGUxloVL3DkuMhqsn0nyMrIkCIWsVVu_%407748428072881B60_0000SID&WebEnvRq=1)]

The synthesis of ^18^F-F-CP was described in detail by Lacan et al. (12). Briefly, modified procedures were used to produce 2-[(2-chloro-2’-fluorodiethyl)amino]-2H-1,3,2-oxazaphosphorinane-2-oxide (12). A halogen exchange reaction was performed with this compound to obtain ^18^F-F-CP. To do this, ^18^F-fluorine exchange was carried out in the presence of ^18^F^–^, potassium bicarbonate, and acetonitrile with Kryptofix 222 at 110°C for 10 min. The total synthesis time was 60–75 min, and the labeling yield at the end of bombardment was 1.1–4.9% (from 16 batches). The radiochemical purity of ^18^F-F-CP was determined by high-performance liquid chromatography to be >99%, and the specific activity was 54–960 Ci/mmol (1.45–25.94 BGq/mmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+F+CP+in+vitro&WebEnv=0GM7xbLRpqXYleVHKSrdtcoA2YyNEqKRHu1LIX7g7EZCk9keIdb3OJDK2qVCir9dELy4Abs87iGdt5K%407748428072881B60_0000SID&WebEnvRq=1)]

The in vitro cytotoxicity of ^18^F-F-CP was compared to that of CP with MCF-7 cells (of human breast cancer origin) using a cell proliferation assay (14). The drug was activated with human liver microsomes as described by the investigators. The cells were subsequently exposed to different concentrations of the activated drugs for 24 h and assayed for cell proliferation. Cytotoxicity of the activated drugs was also compared to that of the pro-drugs. Both CP and ^18^F-F-CP were observed to be significantly more toxic to the cells after activation compared to the non-activated versions (P < 0.01). The investigators observed that a nearly 20-fold higher concentration of the non-activated drug was required to achieve the same effect as the metabolically activated compounds (14).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+F+CP+rodentia&WebEnv=0rVuNvNUw0naLQWUP0ofit0tjpHAFDqhYpIDgY48oV6Mbmz29giqO1RHVQiNZNMP9J79RfEsWixu0-k%407748428072881B60_0000SID&WebEnvRq=1)]

The biodistribution of ^18^F-F-CP was investigated in nude mice bearing MCF-7 cell xenograft tumors (14). Mice (n = 8) were injected intraperitoneally with the labeled CP, and the animals were euthanized after 1 h. The biodistribution of ^18^F-F-CP was also investigated in another group of mice (n = 8) injected with different concentrations of unlabeled CP before treatment with the labeled compound. The visceral organs and blood were collected from each animal of the two respective groups, and they were weighed and counted for incorporation of radioactivity. The uptake after injecting ^18^F-F-CP into the animals was also assessed by positron emission tomography (PET) imaging.

The uptake of ^18^F-F-CP, after injection into the animals, was observed primarily in those organs that were related to the metabolism and excretion of the drug (14). Highest uptake of the label was observed in the kidneys and followed by the liver; the lowest uptake was observed in the brain, and intermediate levels were detected in the tumors. The tumor/tissue and tumor/blood ratios of the labeled drug were not reported. The investigators reported that biodistribution of the labeled drug as observed by PET imaging correlated well with the activity detected in the various harvested organs. They also observed that administration of ~700-fold excess of cold CP did not change the distribution kinetics of the labeled drug in the animals. In addition, the degree of ^18^F-F-CP uptake by the tumor was observed to predict the degree of subsequent response to CP administration to the animal.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+F+CP+Non-Primate+Mammals&WebEnv=0eG1-5HIIbeMtwbeJocRYqJIrBez1qfXhCdpcoIkOXApShINfXj2ow1Rgk5GdeJQ0xKdGGjsUM38erU%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+F+CP+Non+human+primates&WebEnv=0_grzgHsWTXCJtM8jBXOYKmycKwN_b0jxcOLszWRsOu5Bst-DFeTMufOQuoDPDW2u43G_wg653AbvDk%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+F+CP+human+studies&WebEnv=0xcfteT5dQsv3uJIEGmev5eYGGKbCo3ZSH8_r7tUM6UsQW9Wtt8dEYD8X_6_ii3VLWbZiIAVqSEJpfH%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## References

1 Kotter I., Daikeler T., Amberger C., Tyndall A., Kanz L. (2005). Autologous stem cell transplantation of treatment-resistant systemic vasculitis--a single center experience and review of the literature. Clin Nephrol.
2 Marder W., McCune W.J. (2007). Advances in immunosuppressive therapy. Semin Respir Crit Care Med.
3 Muraro P.A., Bielekova B. (2007). Emerging therapies for multiple sclerosis. Neurotherapeutics.
4 Scheinfeld N. (2007). A brief primer on treatments of cutaneous T cell lymphoma, newly approved or late in development. J Drugs Dermatol.
5 Malet-Martino M., Gilard V., Martino R. (1999). The analysis of cyclophosphamide and its metabolites. Curr Pharm Des.
6 Rodriguez-Antona C., Ingelman-Sundberg M. (2006). Cytochrome P450 pharmacogenetics and cancer. Oncogene.
7 Ludeman S.M. (1999). The chemistry of the metabolites of cyclophosphamide. Curr Pharm Des.
8 Sladek N.E., Kollander R., Sreerama L., Kiang D.T. (2002). Cellular levels of aldehyde dehydrogenases (ALDH1A1 and ALDH3A1) as predictors of therapeutic responses to cyclophosphamide-based chemotherapy of breast cancer: a retrospective study. Rational individualization of oxazaphosphorine-based cancer chemotherapeutic regimens. Cancer Chemother Pharmacol.
9 Gamcsik M.P., Dolan M.E., Andersson B.S., Murray D. (1999). Mechanisms of resistance to the toxicity of cyclophosphamide. Curr Pharm Des.
10 Wu L., Tannock I.F. (2003). Repopulation in murine breast tumors during and after sequential treatments with cyclophosphamide and 5-fluorouracil. Cancer Res.
11 Sladek N.E. (1999). Aldehyde dehydrogenase-mediated cellular relative insensitivity to the oxazaphosphorines. Curr Pharm Des.
12 Lacan G., Kesner A.L., Gangloff A., Zheng L., Czernin J., Melega W.P., Silverman D.H.S. (2005). Synthesis of 2-[(2-chloro-2’-18F-fluorodiethyl)amino]-2H-1,3,2-oxazaphosphorinane-2-oxide (18F-fluorocyclophosphamide), a potential tracer for breast tumor prognostic imaging with PET. J Label Compd Radiopharm.
13 Foster A.B., Jarman M., Kinas R.W., van Maanen J.M., Taylor G.N., Gaston J.L., Parkin A., Richardson A.C. (1981). 5-Fluoro- and 5-chlorocyclophosphamide: synthesis, metabolism, and antitumor activity of the cis and trans isomers. J Med Chem.
14 Kesner A.L., Hsueh W.A., Htet N.L., Pio B.S., Czernin J., Pegram M.D., Phelps M.E., Silverman D.H. (2007). Biodistribution and Predictive Value of 18F-Fluorocyclophosphamide in Mice Bearing Human Breast Cancer Xenografts. J Nucl Med.